# 5-[^76^Br]-N-(4-(3,4-Dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl)-2,3-dimethoxybenzamide

Chemical name: | 5-[^76^Br]-N-(4-(3,4-Dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl)-2,3-dimethoxybenzamide
Abbreviated name: | [^76^Br]RHM-4, [^76^Br]1
Synonym:
Agent category: | Compound
Target: | σ_2_ sigma receptor
Target category: | Receptor
Method of detection: | positron emission tomography (PET)
Source of signal: | ^76^Br
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine)]

Sigma receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs such as the liver, kidneys, and endocrine glands (1, 2). The CNS sigma receptors are unique binding sites related to higher brain function. There are at least two subtypes of sigma receptors, σ_1_ and σ_2_ receptors. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (3, 4). The σ_1_ receptors appear to play in a role in motor function and CNS disorders. The σ_2_ receptors, linked to potassium channels and calcium release, are also implicated in malignant cancers (5-7). The density of σ_2_ receptors in tumor cells was found to be greater than that of σ_1_ receptors in tumor cells. The density of σ_2_ receptors was found to be 10-fold higher in proliferating versus quiescent mouse mammary adenocarcinoma cells. Furthermore, σ_2_ receptor ligands were observed to induce apoptosis in tumor cells. Because of these effects, sigma receptor ligands may be useful for detection and treatment in neurology and oncology.

5-[^76^Br]-N-(4-(3,4-Dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl)-2,3-dimethoxybenzamide ([^76^Br]RHM-4), a conformationally flexible benzamide analog, has been shown to have a high affinity (K_i_ = 8.2 nM) and selectivity (σ_2_/σ_1_ ratio > 1573) for σ_2_ receptors on rat liver membranes (8). [^76^Br]RHM-4 (^76^Br t_1/2_ = 16.2 h) has been evaluated as a positron emission tomography (PET) agent for imaging breast tumor in mice (9).

### Related Resource Links:

- Chapters in MICAD (Sigma receptors (http://www.ncbi.nlm.nih.gov/books?term=sigma%20receptors%20AND%20micad%5Bbook%5D), RHM-1/4 (http://www.ncbi.nlm.nih.gov/books?term=RHM%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Sigma receptors (http://www.ncbi.nlm.nih.gov/gene/10280))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Sigma receptors (http://omim.org/entry/601978?search=opoid%20sigma%20receptor&highlight=sigma%20opoid%20receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20synthesis)]

Rowland et al. (9) reported the synthesis of [^76^Br]RHM-4 by a standard electrophilic destannylation reaction of N-[2-(6,7-dimethoxy-3,4-dihydro-1H-isoquinolin-2-yl)-butyl]-2-methoxy-5-(tributylstannyl)benzamide with ^76^Br in NH_4_OH, followed by addition of peracetic acid in dilute acetic acid. High-pressure liquid chromatographic separation gave radiochemical yields of 47–76% (n = 7), with a radiochemical purity >99%. The average specific activity was 40.33 GBq/μmol (1.09 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20in%20vitro)]

Rowland et al. (9) reported that [^76^Br]RHM-4 had an affinity constant (K_d_) of 1.43 ± 0.09 nM and a σ_2_ receptor density (B_max_) of 1,800 ± 83 fmol/mg protein for EMT-6 mouse breast tumors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20rodentia)]

Rowland et al. (9) performed biodistribution studies in EMT-6 tumor–bearing mice showing high accumulation of radioactivity in the kidney [31.2% injected dose per gram (ID/g)], followed by the lung (24.64% ID/g), spleen (12.50% ID/g), liver (10.99% ID/g), and heart (7.31% ID/g) at 5 min after injection of [^76^Br]RHM-4. Tumor accumulation of [^76^Br]RHM-4 was 4.78% ID/g at 5 min, 5.31% ID/g at 30 min, 3.98% ID/g at 60 min, and 1.71% ID/g at 120 min after injection. The liver and kidney showed higher initial uptake than the tumors, with rapid clearances to 1.67% and 1.85% ID/g at 120 min, respectively. Coinjection of [^76^Br]RHM-4 with YUN 143 (a high-affinity σ_2_ and σ_1_ ligand, 1 mg/kg) decreased the tumor, liver, and kidney accumulation significantly (P < 0.005) to 0.98%, 1.38%, and 1.28% ID/g at 120 min, respectively. Another study comparing the tumor uptake and tumor/tissue ratios of [^76^Br]RHM-4 with those of 3'-deoxy-3'-[^18^F]fluorothymidine (http://www.ncbi.nlm.nih.gov/books/NBK23373/) ([^18^F]FLT), a radiolabeled nucleoside analog for measuring tumor proliferation, was also conducted. It was found that [^18^F]FLT had a higher tumor uptake (3.05 ± 0.49% ID/g) than [^76^Br]RHM-4 (1.71 ± 0.17% ID/g) at 120 min. However, [^76^Br]RHM-4 had better tumor/tissue ratios than [^18^F]FLT in the tissues of brain, muscle, fat, heart, bone, blood, and lung. PET imaging studies also showed a higher contrast of the tumor/background tissues with [^76^Br]RHM-4 than with [^18^F]FLT, and YUN 143 decreased accumulation of [^76^Br]RHM-4 in the tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20bromine%20and%20human)]

No publication is currently available.

## Human Studies

F32 CA88487, P30 CA91842, R24 CA86307, R33 CA102869-01

## References

1 Bowen W.D. (2000). Sigma receptors: recent advances and new clinical potentials. Pharm Acta Helv.
2 Walker J.M., Bowen W.D., Walker F.O., Matsumoto R.R., De Costa B., Rice K.C. (1990). Sigma receptors: biology and function. Pharmacol Rev.
3 Mishina M., Ishiwata K., Ishii K., Kitamura S., Kimura Y., Kawamura K., Oda K., Sasaki T., Sakayori O., Hamamoto M., Kobayashi S., Katayama Y. (2005). Function of sigma1 receptors in Parkinson's disease. Acta Neurol Scand.
4 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
5 Colabufo N.A., Berardi F., Contino M., Ferorelli S., Niso M., Perrone R., Pagliarulo A., Saponaro P., Pagliarulo V. (2006). Correlation between sigma2 receptor protein expression and histopathologic grade in human bladder cancer. Cancer Lett.
6 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
7 Wheeler K.T., Wang L.M., Wallen C.A., Childers S.R., Cline J.M., Keng P.C., Mach R.H. (2000). Sigma-2 receptors as a biomarker of proliferation in solid tumours. Br J Cancer.
8 Mach R.H., Huang Y., Freeman R.A., Wu L., Vangveravong S., Luedtke R.R. (2004). Conformationally-flexible benzamide analogues as dopamine D3 and sigma 2 receptor ligands. Bioorg Med Chem Lett.
9 Rowland D.J., Tu Z., Xu J., Ponde D., Mach R.H., Welch M.J. (2006). Synthesis and in vivo evaluation of 2 high-affinity 76Br-labeled sigma2-receptor ligands. J Nucl Med.